# [^18^F]Fluoroethylcholine

Chemical name: | [^18^F]Fluoroethylcholine
Abbreviated name: | [^18^F]FECh
Synonym: | 2-[^18^F]Fluoroethylcholine
Agent category: | Compound
Target: | Choline kinases
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine)]

Choline is an important component of phospholipids in cell membranes. Increased metabolism in tissues will lead to an increased uptake of choline. Choline is phosphorylated by choline kinases (CHK) to phosphorylcholine within cells and, after several biosynthetic processes, is finally integrated into phospholipids (1). Because tumor cells have a high metabolic rate, choline uptake is high in order to keep up with the demands of the synthesis of phospholipids in their cellular membranes (2).

Positron emission tomography (PET) with [^11^C]choline (http://www.ncbi.nlm.nih.gov/books/NBK23549/#Choline11C) has been reported to be useful for the detection and differential diagnosis of brain tumors, prostate cancer, lung cancer, and esophageal cancer (3). However, [^11^C]choline has a high uptake in the liver, kidney, and spleen. An ^18^F-labeled choline analog was initially synthesized as [^18^F]fluoroethylcholine ([^18^F]FECh) to replace [^11^C]choline as a PET tracer due to the short physical half-life of ^11^C (20 min) (4). Although ^18^F has a longer half-life (110 min), [^18^F]FECh exhibited rapid accumulation in the urinary bladder, rendering it less desirable for imaging prostate cancer and pelvic lymph nodes. Therefore, [^18^F]fluorocholine (FCH (http://www.ncbi.nlm.nih.gov/books/NBK23563/#Choline18F)) was conceived to be a better biological analog than [^18^F]FECh (5). PET studies with FCH showed high uptake in malignancies in patients with prostate cancer, breast carcinoma, and brain tumors (6, 7). Choline is also metabolized by choline oxidase in competition with CHK to choline betaine (8), which cannot be phosphorylated by CHK.

### Related Resource Links:

- Chapters in MICAD (Choline (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=choline+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Choline kinase (http://www.ncbi.nlm.nih.gov/gene/1119))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Choline kinase (http://www.ncbi.nlm.nih.gov/omim/612395))
- Clinical trials (Fluorocholine (http://www.clinicaltrials.gov/ct2/results?term=fluorocholine))
- Drug information in FDA (Fluorocholine (http://google2.fda.gov/search?q=fluorocholine&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine%20and%20synthesis)]

An automated method of [^18^F]FECh synthesis was achieved with two-step reactions (9). 2-[^18^F]fluoroethyl tosylate was first prepared by reaction of [^18^F]fluoride with 1,2-bis(tosyloxy)ethane in the presence of tetrabutylammonium carbonate for 8 min at 100°C. 2-[^18^F]Fluoroethyl tosylate was reacted with dimethylethanolamine for 10 min at 100°C. [^18^F]FECh was eluted from a sterile cation-exchange cartridge with saline. The total time required for obtaining the finished chemical was 65 min from the end of bombardment. The radiochemical yield (decay-corrected) was ~40%, with a radiochemical purity of >98%. The specific activity of [^18^F]FECh chloride was 74 MBq/nmol (2 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine%20AND%20in%20vitro)]

[^18^F]FECh was rapidly consumed by yeast choline kinase and bacterial choline oxidase in vitro to form phosphoryl-[^18^F]FECh and [^18^F]FECh betaine (9), respectively. Ehrlich ascites tumor cells converted ~18% of [^18^F]FECh to phosphoryl-[^18^F]FECh with no detectable [^18^F]FECh betaine for 30 min at 37°C. Phosphatidyl-[^18^F]FECh was identified in the tumor cellular membrane homogenates.

## Animal Studies

### Rodent Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine%20AND%20rodentia)]

[^11^C]Choline and [^18^F]FECh PET scans were compared in an animal model of hepatocellular carcinoma (HCC) in woodchucks (n = 6) (10). The size of HCC foci in the liver was 1.0–1.6 cm, with mean tumor/background contrast values of 1.3 ± 0.2 with [^18^F]FECh and 1.5 ± 0.2 with [^11^C]choline at 50 min after injection. The tracers show similar patterns of accumulation immediately after injection, and both radioactivities plateaued at 10 min after injection.

### Other Non-Primate Mammal Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primate Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine%20AND%20primate%20NOT%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fluoroethylcholine%20AND%20human)]

Hara et al. (9) performed a preliminary PET study in one prostate cancer patient after injection of 370 MBq (10 mCi) [^18^F]FECh. [^18^F]FECh was cleared from blood within 5 min after administration. The highest radioactivity was found in the urinary bladder, followed by the kidney and liver. Little radioactivity was found in the bones. The standard uptake values (SUV) were 2.87 at 1.5 min and 4.43 at 55 min after injection. In another study, PET static scans with [^18^F]FECh and [^11^C]choline were performed in 16 patients with untreated primary prostate cancer. The tumor SUV was 3.84 ± 1.25 at 30 min and 4.02 ± 1.46 at 60 min after injection of [^18^F]FECh. For [^11^C]choline, the tumor SUV was 4.03 ± 1.38 at 5 min and 4.50 ± 1.56 at 20 min after injection. PET with [^18^F]FECh showed sharper images of the tumors than did PET with [^11^C]choline. However, a urinary catheter was used to remove urine during the time of PET scanning with [^18^F]FECh.

Steuber et al. (11) performed PET/CT scans with [^18^F]FECh for the detection of lymph node metastasis in 20 high-risk prostate cancer patients prior to radical prostatectomy. Overall, 31 lymph nodes (0.8–12 mm) were identified as positive out of 285 lymph nodes examined after dissection. However, PET/CT scans with [^18^F]FECh did not detect a single positive lymph node before radical prostatectomy.

## NIH Support

R01 CA095307

## References

1 Zeisel S.H., Blusztajn J.K. (1994). Choline and human nutrition. Annu Rev Nutr.
2 Podo F. (1999). Tumour phospholipid metabolism. NMR Biomed.
3 Hara T. (2002). 11C-choline and 2-deoxy-2-[18F]fluoro-D-glucose in tumor imaging with positron emission tomography. Mol Imaging Biol.
4 Hara T., Yuasa M. (1997). Automated synthesis of fluorine-18 labeled choline analogue: 2-fluoroetheyl-dimethyl-2-oxyethylammonium. J Nucl Med.
5 DeGrado T.R., Coleman R.E., Wang S., Baldwin S.W., Orr M.D., Robertson C.N., Polascik T.J., Price D.T. (2001). Synthesis and evaluation of 18F-labeled choline as an oncologic tracer for positron emission tomography: initial findings in prostate cancer. Cancer Res.
6 DeGrado T.R., Baldwin S.W., Wang S., Orr M.D., Liao R.P., Friedman H.S., Reiman R., Price D.T., Coleman R.E. (2001). Synthesis and evaluation of (18)F-labeled choline analogs as oncologic PET tracers. J Nucl Med.
7 Hara T., Kondo T., Hara T., Kosaka N. (2003). Use of 18F-choline and 11C-choline as contrast agents in positron emission tomography imaging-guided stereotactic biopsy sampling of gliomas. J Neurosurg.
8 Ueland P.M. (2011). Choline and betaine in health and disease. J Inherit Metab Dis.
9 Hara T., Kosaka N., Kishi H. (2002). Development of (18)F-fluoroethylcholine for cancer imaging with PET: synthesis, biochemistry, and prostate cancer imaging. J Nucl Med.
10 Kolthammer J.A., Corn D.J., Tenley N., Wu C., Tian H., Wang Y., Lee Z. (2011). PET imaging of hepatocellular carcinoma with (18)F-fluoroethylcholine and (11)C-choline. Eur J Nucl Med Mol Imaging.
11 Steuber T., Schlomm T., Heinzer H., Zacharias M., Ahyai S., Chun K.F., Haese A., Klutmann S., Kollermann J., Sauter G., Mester J., Mikecz P., Fisch M., Huland H., Graefen M., Salomon G. (2010). [F(18)]-fluoroethylcholine combined in-line PET-CT scan for detection of lymph-node metastasis in high risk prostate cancer patients prior to radical prostatectomy: Preliminary results from a prospective histology-based study. Eur J Cancer.